# ^177^Lu-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-human serum albumin-Ac-Cys-Z_EGFR:1907_

Chemical name: | ^177^Lu-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-human serum albumin-Z_EGFR:1907_
Abbreviated name: | ^177^Lu-DO3A-HSA-Z_EGFR:1907_
Synonym:
Agent category: | Antibody, Affibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab -F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A was constructed (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The EGFR-specific Affibody Z_EGFR:1907_ (6.7 kDa) was identified to have good affinity (K_d_ = 5.4 nM) for EGFR (HER1) and labeled with ^111^In via isothiocyanate-benzoyl-diethylenetriaminepentaacetic acid (DTPA) to form ^111^In-Bz-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/) for single-photon emission computed tomography (SPECT) imaging in nude mice bearing human tumors (18). To facilitate site-specific conjugation, Ac-Cys-Z_EGFR:1907_ (Cys at the N terminal) was synthesized and conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7-tris-aceticacid-10-maleimidethylacetamide (maleimido-mono-amide-DOTA) to form Ac-Cys(DOTA)-Z_EGFR:1907_ (DOTA-Z_EGFR:1907_) and labeled with ^64^Cu (t_1/2_, 12.7 h) to form ^64^Cu-DOTA-Z_EGFR:1907_ for positron emission tomography imaging studies in tumor-bearing mice (19). Although high specific tumor accumulation was observed with ^111^In- and ^64^Cu-labeled Z_EGFR:1907,_ very high kidney accumulation (>100% injected dose per gram (ID/g)) was also observed. Addition of human serum albumin (HSA) to Affibody Z_HER2:342_ dramatically reduced kidney accumulation and improved tumor accumulation (20). Therefore, Hoppmann et al. (21) prepared ^177^Lu-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid-human serum albumin-Z_EGFR:1907_ (^177^Lu-DO3A-HSA-Z_EGFR:1907_) for use in SPECT imaging of EGFR in nude mice bearing human solid tumors showing good tumor contrast but low kidney accumulation.

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR+1907+synthesis)]

Ac-Cys-Z_EGFR:1907_ was prepared with automated solid-phase peptide synthesizer (21). DOTA-N-hydroxysuccinimide eater and HSA (100:1 molar ratio) were incubated in borate buffer (pH 8.5) for 2 h at 4°C to form DO3A-HSA, which was isolated with PD-10 column. DO3A-HSA was then reacted with sulfosuccinimidyl 4-[N-maleimidomethyl]cyclohexane-1-carboxylate (Sulfo-SMCC) in molar ratio of 1:5 for 1 h at 4 °C. The resulting bioconjugate was further purified using the PD-10 column. Ac-Cys-Z_EGFR:1907_ was site specifically conjugated to the DOTA and Sulfo-SMCC modified HSA via the cysteine residue. The reaction was performed in a molar ratio of 1:5 of DO3A-HSA-SMCC and Ac-Cys-Z_EGFR:1907_ (22 nmol) for 6 h at room temperature. DO3A-HSA-Z_EGFR:1907_ was purified with ultracentrifugation. There were average three DO3A moieties and two Ac-Cys-Z_EGFR:1907_ moieties per HSA protein as determined with MALDI-TOF-MS and sodium dodecyl sulfate polyacrylamide gel electrophoresis (SDS-PAGE). Approximately 2.4 nmol of the DO3A-HSA-Z_EGFR:1907_ was radiolabeled with ^64^Cu by addition of 74 MBq (2 mCi) of ^177^LuCl_3_ in 0.1 N sodium acetate buffer (pH 5.0) and incubated for 1 h at 39°C. ^177^Lu-DO3A-HSA-Z_EGFR:1907_ was isolated with PD-10 column with >70% radiolabeling yield. ^177^Lu-DO3A-HSA-Z_EGFR:1907_ exhibited a specific activity of ~30 MBq/nmol (1.0 mCi/nmol) at the end of synthesis. ^177^Lu-DO3A-HSA-Z_EGFR:1907_ was >95% intact in mouse serum for 4 h at 37°C and >80% intact at 24-168 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20in%20vitro)]

Accumulation studies of ^177^Lu-DO3A-HSA-Z_EGFR:1907_ in SAS human oral squamous carcinoma cells were measured at 37°C (total cell-associated radioactivity) and 4°C (membrane-bound radioactivity) at 0.5-4 h of incubation (21). Total cell-associated radioactivity was 1.97 ± 0.08% incubation dose(ID) at 0.5 h and 8.43 ± 0.55% ID at 4 h, whereas membrane-bound radioactivity was 4-fold to 5-fold lower than the total cell-associated radioactivity. Excess unlabeled Ac-Cys-Z_EGFR:1907_ inhibited the accumulation at all incubation time points. There were 80% and 65% inhibition at 37°C and 4°C at 4 h, respectively. ^177^Lu-DO3A-HSA-Z_EGFR:1907_ exhibited 1.5%, 7.9%, and 38.7% internalization of ID at 1 min, 30 min and 24 h, respectively. On the other hand, ^177^Lu-DO3A-Z_EGFR:1907_ exhibited 2.3%, 9.6%, and 28.9% internalization of ID at 2 min, 30 min and 24 h, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20rodentia)]

Hoppmann et al. (21) performed ex vivo biodistribution studies of ^177^Lu- DO3A-HSA-Z_EGFR:1907_ in mice (n = 4/group) bearing SAS tumors with tumor accumulation of 2.0 ± 0.8% injected dose per gram (ID/g), 3.1 ± 1.0% ID/g, 4.6 ± 0.2% ID/g, 5.2 ± 0.7% ID/g, 5.3 ± 0.4% ID/g, 3.7 ± 0.6% ID/g, and 3.1 ± 1.0% ID/g at 1, 4, 24, 48, 72, 120, and 240 h after injection, respectively. The organ with the highest radioactivity was the liver (54.9% ID/g), followed by the blood (19.1% ID/g), kidney (11.1% ID/g), spleen (~12% ID/g), lung (~7% ID/g), and muscle (<1.0% ID/g) at 4 h after injection. ^177^Lu-DO3A-HSA-Z_EGFR:1907_ exhibited a two-phase blood clearance kinetics with distribution and elimination half-life of 1.99 and 25.5 h, respectively. The tumor/muscle ratio increased from 3.3 at 1 h to 7.9 at 72-240 h, whereas the tumor/blood ratio increased from 1.7 at 48 h to 16.7 at 240 h. No blocking studies were performed.

SPECT static imaging analysis was performed in nude mice (n = 3) bearing SAS tumors at 4, 24, 48, and 72 h after intravenous injection of 7.4-11.1 MBq (0.2-0.0.3 mCi) ^177^Lu-DO3A-HSA-Z_EGFR:1907_ (~0.5 nmol) (21). The tumor was clearly visualized at 24-72 h. High accumulation levels were observed in the liver at 4-72 h. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## NIH Support

5R01 CA119053, P50 CA114747

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
19 Miao Z., Ren G., Liu H., Jiang L., Cheng Z. (2010). Small-animal PET imaging of human epidermal growth factor receptor positive tumor with a 64Cu labeled affibody protein. Bioconjug Chem.
20 Hoppmann S., Miao Z., Liu S., Liu H., Ren G., Bao A., Cheng Z. (2011). Radiolabeled affibody-albumin bioconjugates for HER2-positive cancer targeting. Bioconjug Chem.
21 Hoppmann S., Qi S., Miao Z., Liu H., Jiang H., Cutler C.S., Bao A., Cheng Z. (2012). (177)Lu-DO3A-HSA-Z (EGFR:1907): characterization as a potential radiopharmaceutical for radionuclide therapy of EGFR-expressing head and neck carcinomas. J Biol Inorg Chem.